# Galactosamine-serum albumin-rhodamineX_20_

Chemical name: | Galactosamine-serum albumin-rhodamineX_20_
Abbreviated name: | GmSA-20ROX
Synonym:
Agent Category: | Polypeptide
Target: | β-D-galactose receptor
Target Category: | Receptor binding
Method of detection: | Optical fluorescence imaging
Source of signal: | RhodamineX
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GmSA-20ROX)]

Optical fluorescence imaging is increasingly used to study biological functions of specific targets (1, 2). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have a wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging in small animals.

A variety of cancer cells express on their cell surface receptors (lectins) that bind to glycosylated proteins (3, 4). The β-D-galactose receptor binds and internalizes proteins that contain galactose sugar residues. Galactosamine-serum albumin (GmSA) was labeled with rhodamine green (RhodG) to study in vivo biodistribution of the tracer in tumor-bearing mice and was found to have a high accumulation in a variety of human ovarian adenocarcinomas in nude mice (5). A self-quenching GmSA complex was create by conjugating 20 rhodamineX (ROX) molecules to GmSA (GMSA-rhodamineX_20_ (GmSA-20ROX)) (6). ROX is an optical fluorescence dye with an absorbance maximum at 595 nm and an emission maximum at 610 nm. GmSA-20ROX was found to have a high accumulation in peritoneal micrometastases of human SHIN3 ovarian adenocarcinomas in nude mice (6).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GmSA-20ROX+synthesis)]

Commercially available GmSA (7.0 nmol), which contains 23 galactosamine residues, was incubated with ROX-succinimidyl ester (360 nmol) for 15 min at room temperature (6). GmSA-20ROX was isolated by column chromatography. There were ~20 ROX per GmSA as determined by spectroscopy. GmSA-1ROX was also synthesized using 14 nmol ROX-succinimidyl ester.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GmSA-20ROX+and+in+vitro)]

Flow cytometry and fluorescence microscopy confirmed intracellular accumulation of GmSA-20ROX into SHIN3 cells (6). The mean fluorescence intensity (MFI) for cells treated with GmSA-20ROX progressively increased with time of incubation (0.5–6 h). The rate of MFI increase was 5.574 a.u./h for GmSA-20ROX and 0.485 a.u/h for GmSA-1ROX. GmSA-20ROX became more than five-fold more fluorescent than cells treated with GmSA-1ROX. GmSA-20ROX was bound to the cell surface and internalized into intracellular lysosomes and endosomes where the GmSA-20ROX molecules were unfolded and digested, resulting in increased fluorescence signals because of dequenching. GmSA-20ROX fluorescence was markedly activated by trypsin, cathepsin D, and matrix metalloproteinase 2 (MMP-2), whereas GmSA-1ROX was mildly activated by MMP-2 only.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GmSA-20ROX+rodentia)]

Hama et al. (6) performed studies of GmSA-20ROX in nude mice bearing intraperitoneal (i.p.) xenografts of the SHIN3 cell line. Images were obtained after i.p. injection of 50 μg (~0.7 nmol) GmSA-20ROX or GmSA-1ROX. Higher fluorescence intensity was observed with GmSA-20ROX than with GmSA-1ROX at 1 h and 3 h after injection in the tumors formed in the exposed abdomen. Tumors that were <1 mm in diameter were visible. Sensitivity and specificity for GmSA-20ROX (n = 336 tumor foci) were 99% and 99%, whereas these values were 24% and 100%, respectively, for GmSA-1ROX (n = 388 tumor foci). Ex vivo study of subcellular localization in the tumors was not performed. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GmSA-20ROX+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GmSA-20ROX+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=GmSA-20ROX+human)]

No publication is currently available.

## NIH Support

Intramural Research Program

## References

1 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
2 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
3 Stockert R.J. (1995). The asialoglycoprotein receptor: relationships between structure, function, and expression. Physiol Rev.
4 Hama Y., Urano Y., Koyama Y., Choyke P.L., Kobayashi H. (2006). Targeted optical imaging of cancer cells using lectin-binding BODIPY conjugated avidin. Biochem Biophys Res Commun.
5 Gunn A.J., Hama Y., Koyama Y., Kohn E.C., Choyke P.L., Kobayashi H. (2007). Targeted optical fluorescence imaging of human ovarian adenocarcinoma using a galactosyl serum albumin-conjugated fluorophore. Cancer Sci.
6 Hama Y., Urano Y., Koyama Y., Gunn A.J., Choyke P.L., Kobayashi H. (2007). A Self-Quenched Galactosamine-Serum Albumin-RhodamineX Conjugate: A "Smart" Fluorescent Molecular Imaging Probe Synthesized with Clinically Applicable Material for Detecting Peritoneal Ovarian Cancer Metastases. Clin Cancer Res.